# Radioiodinated anti-TAG-72 humanized C_H_2 domain-deleted antibody

Chemical name: | Radioiodinated anti-TAG-72 humanized C_H_2 domain-deleted antibody
Abbreviated name: | Radioiodinated HuCC49ΔC_H_2 Ab
Synonym: | ^125^I-HuCC49ΔC_H_2 Ab, ^125^I-CC49 Ab, ^131^I-HuCC49ΔC_H_2 Ab, ^131^I-CC49 Ab
Agent Category: | Humanized C_H_2 domain-deleted antibody variant
Target: | (Sialyl-Tn) TAG-72
Target Category: | Antibody to antigen binding
Method of detection: | Single-photon emission computed tomography (SPECT), planar gamma imaging
Source of signal: | ^125^I, ^131^I
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=144964805), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=21689921) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=182875&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about TAG-72

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HuCC49DeltaC(H)2)+OR+(chimeric+domain-deleted+anticarcinoma+immunoglobulins)+OR+(CDR-grafted+domain-deleted+antitumor+antibody))]

Radioiodinated anti-TAG-72 humanized C_H_2 domain-deleted antibody (radioiodinated HuCC49ΔC_H_2 Ab), which is formed by the conjugation of radioactive iodine (^125^I or ^131^I) with a bioengineered anti–tumor-associated glycoprotein 72 (TAG-72) antibody construct, has been developed for gamma imaging of cancers that express TAG-72 (1-4). ^125^I has a physical half-life (t_½_) of 60 days, and ^131^I has a t_½_ of 8 days.

The TAG-72 antigen was isolated from the LS-174T human colon cancer xenograft as a high molecular weight glycoprotein (molecular mass of 10^6^ Da) with mucin-like characteristics (3, 5-7). It is expressed on a variety of human adenocarcinomas such as pancreatic, breast, colorectal, prostate, endometrial, and ovarian cancers. This antigen has also been shown to be shed into the serum of cancer patients (8). The murine monoclonal antibody B72.3 (MAb B72.3) against TAG-72 was initially generated by immunization of mice with a membrane-enriched fraction of a human breast carcinoma (9). With use of affinity-purified TAG-72 from LS-174T as an immunogen, CC49 and other anti–TAG-2 MAbs with higher affinity constants (K_a_) have been produced and characterized (5, 6, 9, 10). To optimize the pharmacokinetics of CC49 MAb, Hutzell et al. (11) generated a recombinant chimeric B72.3 (cCC49) with a human γ_1_ constant region. Whittle et al. (12) also reported the preparation of a cCC49 Ab with a human γ_4_ constant region. Faster plasma clearance of cCC49 Ab was seen in mice, but similar results were not observed in monkeys and humans.

Radiolabeled MAbs have been developed for both the diagnosis and treatment of tumors (13). Radiolabeled B72.3 and CC49 (intact IgGs) have shown excellent tumor localization capabilities with potential diagnostic and therapeutic applications in the clinical setting (14, 15). Because of their relatively large size, radiolabeled intact MAbs tend to have unfavorable imaging kinetics, poor tumor penetration, and high potential for human anti-mouse antibody response (10, 16-18). The removal of the C_H_2 domain of IgG appears to result in a significantly faster blood clearance and more rapid tumor uptake (19-21). Slavin-Chiorini et al. (1) bioengineered a complementary determining region-grafted humanized CC49 MAb (HuCC49) with a C_H_2 domain deletion (ΔC_H_2). The light chain constant domain was a human Cκ, and the human γ_1_ chain was genetically modified to produce a heavy chain composed of a C_H_1 domain followed by a partial IgG_1_ hinge region tethered to the C_H_3 heavy chain domain by addition of a flexible 10-amino-acid GGGSSGGGSG spacer (22). The structure of HuCC49ΔC_H_2 was investigated by Larson et al. (23), and they reported that the antigen combining site of HuCC49ΔC_H_2 was very similar, but not identical, in topology and charge distribution to that of B72.3. Radioiodinated (^125^I or ^131^I) HuCC49ΔC_H_2 constructs have demonstrated faster blood clearance in mice (1, 21, 24). Clinical studies in patients showed potential applications of radioiodinated HuCC49ΔC_H_2 Ab (2-4).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HuCC49DeltaC(H)2)+OR+(chimeric+domain-deleted+anticarcinoma+immunoglobulins)+OR+(CDR-grafted+domain-deleted+antitumor+antibody))]

Slavin-Chiorini et al. (1) first reported the preparation and radiolabeling of ^131^I-HuCC49ΔC_H_2 Ab. The HuCC49 Ab was prepared by grafting the CC49 MAb hypervariable regions onto the variable light and variable heavy frameworks of the human MAbs LEN and 21/28’ CL, respectively. The HuCC49ΔC_H_2 heavy and light chain expression constructs were introduced by sequential electroporation into the SP2/0-Ag14 cell line. HuCC49ΔC_H_2 was then purified by filtration and dialysis from the bioreactor supernatant. Purified HuCC49ΔC_H_2 was labeled with either Na^125^I or Na^131^I using the standard 1,3,4,6-tetrachloro-3α,6α-diphenylglycoluril (IodoGen) method. The labeling conditions, radiochemical yield, and radiochemical purity were not reported. The specific activity was 74–185 kBq/μg (2–5 μCi/μg) or 11.3–28.3 kBq/pmol (418.7–1046.6 kBq/pmol) based on a molecular mass of 153 kDa. The average immunoreactivity was reported to be 95%–98%. The molecular mass profile of ^125^I/^131^I-HuCC49ΔC_H_2 was evaluated by autoradiography after SDS-PAGE under non-reducing and reducing conditions. Under non-reducing conditions, the HuCC49ΔC_H_2 migrated as two bands, a major band of 153 kDa and a band of 73 kDa. The band of 153 kDa was consistent with the molecular mass of an IgG with a C_H_2 domain deletion. Size-exclusion chromatography under non-denaturing conditions yielded only one major peak, which corresponded to the C_H_2-deleted HuCC49. Under reducing conditions, the HuCC49ΔC_H_2 was resolved into two bands with molecular masses of 43 and 27 kDa. This was consistent with the molecular masses of an IgG heavy chain with a C_H_2 domain deletion and an intact light chain, respectively.

Liu et al. (25) reported biosynthesis of HuCC49ΔC_H_2 in mammalian Chinese hamster ovary cells produced two homodimeric isoforms (form A and form B) in ~50:50 mixture. Form A was found to be more stable and is the preferred molecule for clinical development. On the basis of this observation, Glaser et al. (22) developed a panel of hinge-engineered HuCC49ΔC_H_2 Abs to produce >98% form A isoform. In human studies with radioiodinated HuCC49ΔC_H_2, the unbound radioactive iodine was removed by ion exchange cartridge or high-performance liquid chromatography (HPLC). The final product was sterilized by filtration. Quality control tests including purity, immunoreactivity, apyrogenicity, and sterility in accordance with the United States Food and Drug Administration regulations were performed before patient administration (2-4). Forero et al. (2) reported a radiochemical efficiency and purity >99.0% by HPLC and an immunoreactivity of 67%–69%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HuCC49DeltaC(H)2)+OR+(chimeric+domain-deleted+anticarcinoma+immunoglobulins)+OR+(CDR-grafted+domain-deleted+antitumor+antibody))]

Slavin-Chiorini et al. (1) conducted in vitro solid-phase competition immunoassays of ^125^I-HuCC49ΔC_H_2 Ab with bovine submaxillary mucin (BSM) as the TAG-72 antigen source. The 50% inhibitory concentration value (IC_50_) was ~1.5–3.5 nM. The apparent affinity constant (K_a_) of unlabeled HuCC49ΔC_H_2 Ab was 5.1 × 10−^9^.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=HuCC49DeltaC(H)2)+OR+(chimeric+domain-deleted+anticarcinoma+immunoglobulins)+OR+(CDR-grafted+domain-deleted+antitumor+antibody))]

Pharmacokinetics studies of radioiodinated-HuCC49ΔC_H_2 Ab were performed in groups of five normal nude mice (1). No thyroid blockage was reported. Each mouse received a mixture of 122.1 kBq (3.3 μCi) of ^131^I-HuCC49ΔC_H_2 Ab and 118.4 kBq (3.2 μCi) ^125^I-HuCC49 Ab by i.v. or i.p. administration. In the i.v. injection group, starting at 0.5 h after administration, ^131^I-HuCC49ΔC_H_2 Ab showed a significantly faster plasma clearance than the intact ^125^I-HuCC49 Ab. About 74% and 99% of ^131^I-HuCC49ΔC_H_2 had cleared the plasma at 6 h and 14 h, respectively. In comparison, 58% and 74% of ^125^I-HuCC49 were cleared at 6 h and 24 h, respectively. In the i.p. injection group, the percentage injected dose per g (% ID/g) radioactivity of ^131^I-HuCC49ΔC_H_2 that moved out of the abdominal cavity and into serum peaked at 2 h while the radioactivity of ^125^I-HuCC49 peaked between 2h and 4 h. Less than 1% of ^131^I-HuCC49ΔC_H_2 radioactivity remained in the plasma at 24 h. In comparison, 3% of ^125^I-HuCC49 radioactivity remained in the plasma at 120 h. Even more pronounced differences in the pharmacokinetic profiles between ^131^I-HuCC49ΔC_H_2 and ^125^I-HuCC49 were found in severely compromised immunodeficient mice by either i.v. or i.p. injection of the radioiodinated Abs.

Slavin-Chiorini et al. (1) performed biodistribution studies of ^131^I-HuCC49ΔC_H_2 in nude mice bearing TAG-72 tumors. No thyroid blockage was reported. Each mouse received a mixture of 122.1 kBq (3.3 μCi) ^131^I-HuCC49ΔC_H_2 and 118.4 kBq (3.2 μCi) intact ^125^I-HuCC49 by i.v. or i.p. administration. In the i.v. injection group (n = 5), the average ^131^I-HuCC49ΔC_H_2 tumor radioactivity levels (% ID/g) were 11.1 (24 h), 10.6 (48 h), 10.3 (72 h), and 5.6 (120 h). The ^125^I-HuCC49 tumor radioactivity levels (% ID/g) were 9.0 (24 h), 11.0 (48 h), 14.2 (72 h), and 18.6 (120 h). The average radiolocalization indices (RI = tumor % ID/g divided by normal tissue % ID/g) of ^131^I-HuCC49ΔC_H_2 for the tumor/blood ratio were 7.4 (24 h), 102.0 (48 h), 226.1 (72 h), and 264.4 (120 h). The tumor/blood RI values for ^125^I-HuCC49 were 1.4 (24 h), 4.9 (48 h), 6.1 (72 h), and 10.6 (120 h). At 24 h, the radioactivity levels (% ID/g) of ^131^I-HuCC49ΔC_H_2 in other major organs were 2.0 (blood), 6.4 (liver), 8.0 (spleen), 1.5 (kidney), and 1.5 (lung). At 120 h, these values changed to 0.0 (blood), 0.1 (liver), 0.3 (spleen), 0.0 (kidney), and 0.0 (lung). In the i.p. injection group, the average ^131^I-HuCC49ΔC_H_2 tumor radioactivity levels (% ID/g) were 5.4 (24 h), 5.6 (48 h), 3.9 (72 h), and 2.8 (120 h). The average tumor/blood ratio RI values were 7.0 (24 h), 51.6 (48 h), 146.5 (72 h), and 409.7 (120 h). In comparison, the average ^125^I-HuCC49 tumor radioactivity levels (% ID/g) were 5.8 (24 h), 10.6 (48 h), 11.0 (72 h), and 18.8 (120 h). The average tumor/blood ratio RI values were 1.2 (24 h), 3.0 (48 h), 4.5 (72 h), and 12.9 (120 h). At 24 h, the radioactivity levels (% ID/g) of ^131^I-HuCC49ΔC_H_2 in other major organs were 0.8 (blood), 2.9 (liver), 2.0 (spleen), 0.6 (kidney), and 0.6 (lung). At 120 h, these values changed to 0.0 (blood), 0.0 (liver), 0.2 (spleen), 0.0 (kidney), and 0.0 (lung).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((HuCC49DeltaC(H)2)+OR+(chimeric+domain-deleted+anticarcinoma+immunoglobulins)+OR+(CDR-grafted+domain-deleted+antitumor+antibody))+AND+(dog+OR+rabbit+OR+pig+OR+sheep))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((HuCC49DeltaC(H)2)+OR+(chimeric+domain-deleted+anticarcinoma+immunoglobulins)+OR+(CDR-grafted+domain-deleted+antitumor+antibody))+AND+(primate+NOT+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=((HuCC49DeltaC(H)2)+OR+(chimeric+domain-deleted+anticarcinoma+immunoglobulins)+OR+(CDR-grafted+domain-deleted+antitumor+antibody))AND+human)]

Agnese et al. (4) conducted a pilot study of ^125^I-HuCC49ΔC_H_2 in 20 patients with recurrent colorectal cancer. After thyroid blockage, each patient received 74 MBq/mg (2 mCi/mg) or 74 MBq/6.54 nmol (2 mCi/6.54 nmol based on a molecular mass of 153 kDa) of ^125^I-HuCC49ΔC_H_2. Surgical operations were performed 3–24 days after injection. During the operation, a radioimmunoguided surgical (RIGS) exploration with a handheld gamma-detecting probe was performed immediately after the traditional exploration. The final study group comprised five patients who underwent exploration when distinction of truly positive tissue from background counts was possible. In the traditional exploration, 9 out of 10 tumor sites (90%) were confirmed by conventional histological methods. In the RIGS exploration, 14 out of 15 tumor sites (93%) were confirmed by pathological studies. There were 5 pathologically confirmed tumor sites identified by RIGS but not identified by traditional exploration. Only 1 pathologically confirmed tumor site was identified by traditional exploration but not by RIGS. None of the patients expressed significant human anti-mouse antibody (HAMA) response after exposure to ^125^I-HuCC49ΔC_H_2.

Forero et al. (2) obtained HuCC49ΔC_H_2 from the National Cancer Institute under its Investigational New Drug Application No. 9260 for study in four patients with TAG-72–positive metastatic colorectal carcinoma. HuCC49ΔC_H_2 was labeled with ^131^I at 370 MBq/mg (10 mCi/mg) or 56.6 kBq/pmol (1.52 μCi/pmol) based on a molecular mass of 153 kDa. With thyroid blockage, unlabeled HuCC49ΔC_H_2 Ab was infused in sufficient amounts to bring the total dose of antibody protein to 20 mg prior to the injection of the ^131^I-HuCC49ΔC_H_2. Each patient received 370 MBq (10 mCi) ^131^I-HuCC49ΔC_H_2 by i.v. infusion. The mean pharmacokinetic parameter values of these 4 patients were 20 ± 2.6 h (serum t_½_), 3.5 ± 0.5 μCi/ml (peak concentration), 10 ± 2 h/μCi/ml (area under the curve), 1.5 ± 0.1 ml/h/kg (clearance), and 43 ± 6 ml/kg (volume of distribution). In comparison, the serum t_½_ of intact ^131^I-murine CC49 was 50 ± 11 h. Gamma imaging of ^131^I-HuCC49ΔC_H_2 showed at least one known tumor site in each patient but fewer tumor sites were consistently detected than those found with conventional x-ray computed tomography scan. Dosimetry studies showed that the mean absorbed doses were 0.135 mGy/MBq (0.5 rad/mCi) for whole body, 0.270 mGy/MBq (rad/mCi) for marrow, 0.621 mGy/MBq (rad/mCi) for liver, 1.081 mGy/MBq (rad/mCi) for kidney, 4.351 mGy/MBq (16.1 rad/mCi) for thyroid, and 2 mGy/MBq (7.4 rad/mCi) for tumor. Immunogenicity studies showed that there was no evidence of antibody response to HuCC49ΔC_H_2 in three patients over a 6-week period, and one patient had a minimal response by week 6. No acute toxicity, bone marrow suppression, or other nonhematologic toxicities were reported in these four patients.

Xiao et al. (3) studied ^125^I-HuCC49ΔC_H_2 in 21 patients with colorectal carcinoma by giving 74 MBq/mg (2 mCi/mg) of the radiolabeled Ab by i.v. bolus. Thyroid blockage was instituted, and each patient underwent exploratory laparotomy 3–20 days after injection. Using precordial detection of radioactivity with a handheld gamma-detecting probe, the ^125^I-HuCC49ΔC_H_2 circulation appeared to fit into a two-compartment open model with first-order elimination from the central compartment. The t_½α_ (day 1 to day 10) and t_½β_ (day 10 to day 20) were ~1.34 and 12.8 days, respectively. Urinary excretion accounted for 63.6 ± 20.3% of the total dose. There appeared to be a linear relationship between the tumor radioactivity level and the circulating radioactivity level. The tumors showed five- to ten-fold higher radioactivity levels above the background (blood and normal organs) over 3–21 days. After 20 days, the radioactivity levels in blood and normal organs decreased to a minimal level. Intestinal primary tumors and metastatic liver tumors had the highest radioactivity levels, whereas the abdominal wall tumors had the lowest levels. No patients showed a HAMA response.

## NIH Support

NIH CURE Program K12-CA76937, R01 Ovarian SPORE CA84152.

## References

1 Slavin-Chiorini D.C., Kashmiri S.V., Lee H.S., Milenic D.E., Poole D.J., Bernon E., Schlom J., Hand P.H. (1997). A CDR-grafted (humanized) domain-deleted antitumor antibody. Cancer Biother Radiopharm.
2 Forero A., Meredith R.F., Khazaeli M.B., Carpenter D.M., Shen S., Thornton J., Schlom J., LoBuglio A.F. (2003). A novel monoclonal antibody design for radioimmunotherapy. Cancer Biother Radiopharm.
3 Xiao J., Horst S., Hinkle G., Cao X., Kocak E., Fang J., Young D., Khazaeli M., Agnese D., Sun D., Martin E. (2005). Pharmacokinetics and clinical evaluation of 125I-radiolabeled humanized CC49 monoclonal antibody (HuCC49deltaC(H)2) in recurrent and metastatic colorectal cancer patients. Cancer Biother Radiopharm.
4 Agnese D.M., Abdessalam S.F., Burak W.E., Arnold M.W., Soble D., Hinkle G.H., Young D., Khazaeli M.B., Martin E.W. (2004). Pilot study using a humanized CC49 monoclonal antibody (HuCC49DeltaCH2) to localize recurrent colorectal carcinoma. Ann Surg Oncol.
5 Muraro R., Kuroki M., Wunderlich D., Poole D.J., Colcher D., Thor A., Greiner J.W., Simpson J.F., Molinolo A., Noguchi P., et al. (1988). Generation and characterization of B72.3 second generation monoclonal antibodies reactive with the tumor-associated glycoprotein 72 antigen. Cancer Res.
6 Johnson V.G., Schlom J., Paterson A.J., Bennett J., Magnani J.L., Colcher D. (1986). Analysis of a human tumor-associated glycoprotein (TAG-72) identified by monoclonal antibody B72.3. Cancer Res.
7 Katari R.S., Fernsten P.D., Schlom J. (1990). Characterization of the shed form of the human tumor-associated glycoprotein (TAG-72) from serous effusions of patients with different types of carcinomas. Cancer Res.
8 Paterson A.J., Schlom J., Sears H.F., Bennett J., Colcher D. (1986). A radioimmunoassay for the detection of a human tumor-associated glycoprotein (TAG-72) using monoclonal antibody B72.3. Int J Cancer.
9 Colcher D., Hand P.H., Nuti M., Schlom J. (1981). A spectrum of monoclonal antibodies reactive with human mammary tumor cells. Proc Natl Acad Sci U S A.
10 Goel A., Baranowska-Kortylewicz J., Hinrichs S.H., Wisecarver J., Pavlinkova G., Augustine S., Colcher D., Booth B.J., Batra S.K. (2001). 99mTc-labeled divalent and tetravalent CC49 single-chain Fv's: novel imaging agents for rapid in vivo localization of human colon carcinoma. J Nucl Med.
11 Hutzell P., Kashmiri S., Colcher D., Primus F.J., Hand P.H., Roselli M., Finch M., Yarranton G., Bodmer M., Whittle N., et al. (1991). Generation and characterization of a recombinant/chimeric B72.3 (human gamma 1). Cancer Res.
12 Whittle N., Adair J., Lloyd C., Jenkins L., Devine J., Schlom J., Raubitschek A., Colcher D., Bodmer M. (1987). Expression in COS cells of a mouse-human chimaeric B72.3 antibody. Protein Eng.
13 Kowalsky R.J., Falen S.W. (2004). and Radiopharmaceuticals in nuclear pharmacy and nuclear medicine, American Pharmacists Association: Washington, D.C. p. 733-752.
14 Colcher D., Minelli M.F., Roselli M., Muraro R., Simpson-Milenic D., Schlom J. (1988). Radioimmunolocalization of human carcinoma xenografts with B72.3 second generation monoclonal antibodies. Cancer Res.
15 Colcher D., Esteban J., Carrasquillo J.A., Sugarbaker P., Reynolds J.C., Bryant G., Larson S.M., Schlom J. (1987). Complementation of intracavitary and intravenous administration of a monoclonal antibody (B72.3) in patients with carcinoma. Cancer Res.
16 Britton K.E. (1990). The development of new radiopharmaceuticals. Eur J Nucl Med.
17 Jain R.K. (1987). Transport of molecules across tumor vasculature. Cancer Metastasis Rev.
18 Primus F.J., Bennett S.J., Kim E.E., DeLand F.H., Zahn M.C., Goldenberg D.M. (1980). Circulating immune complexes in cancer patients receiving goat radiolocalizing antibodies to carcinoembryonic antigen. Cancer Res.
19 Chinn P.C., Morena R.A., Santoro D.A., Kazules T., Kashmiri S.V., Schlom J., Hanna N., Braslawsky G. (2006). Pharmacokinetics and tumor localization of (111)in-labeled HuCC49DeltaC(H)2 in BALB/c mice and athymic murine colon carcinoma xenograft. Cancer Biother Radiopharm.
20 Mueller B.M., Reisfeld R.A., Gillies S.D. (1990). Serum half-life and tumor localization of a chimeric antibody deleted of the CH2 domain and directed against the disialoganglioside GD2. Proc Natl Acad Sci U S A.
21 Slavin-Chiorini D.C., Horan Hand P.H., Kashmiri S.V., Calvo B., Zaremba S., Schlom J. (1993). Biologic properties of a CH2 domain-deleted recombinant immunoglobulin. Int J Cancer.
22 Glaser S.M., Hughes I.E., Hopp J.R., Hathaway K., Perret D., Reff M.E. (2005). Novel antibody hinge regions for efficient production of CH2 domain-deleted antibodies. J Biol Chem.
23 Larson S.B., Day J.S., Glaser S., Braslawsky G., McPherson A. (2005). The structure of an antitumor C(H)2-domain-deleted humanized antibody. J Mol Biol.
24 Slavin-Chiorini D.C. Kashmiri S.V. Schlom J. Calvo B. Shu L.M. Schott M.E. Milenic D.E. Snoy P. Carrasquillo J. Anderson K. Biological properties of chimeric domain-deleted anticarcinoma immunoglobulins Cancer Res 1995 55Suppl23 5957s 5967s 7493377
25 Liu T., Meredith R.F., Saleh M.N., Wheeler R.H., Khazaeli M.B., Plott W.E., Schlom J., LoBuglio A.F. (1997). Correlation of toxicity with treatment parameters for 131I-CC49 radioimmunotherapy in three phase II clinical trials. Cancer Biother Radiopharm.